# 6-[^18^F]Fluorodopamine

Chemical name: | 6-[^18^F]Fluorodopamine
Abbreviated name: | 6-[^18^F]FDA, [^18^F]FDA
Synonym:
Agent category: | Compound
Target: | Sympathetic neuron transporters and dopamine β-hydroxylase
Target category: | Transporter: enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%226-fluorodopamine%22%5BSubstance%20Name%5D)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition and emotion. Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in striatum of the brain (1, 2). Dopamine (DA) is synthesized within nerve cells (3). Chemically, L-tyrosine is converted to dihydroxyphenylalanine (L-DOPA) and then to dopamine in a two-step process. The first, rate limiting step is catalyzed by tyrosine 3-monoxygenase (tyrosine hydroxylase or TH). The second step is catalyzed by aromatic L-amino acid decarboxylase (L-DOPA decarboxylase, AAAD). In dopaminergic neurons, dopamine is not metabolized further, and is stored in vesicles in the presynaptic nerve terminals. Interstitial dopamine is re-captured by dopamine transporter, DAT.

In noradrenergic neurons, dopamine is converted to norepinephrine (NE) by dopamine β-hydroxylase (DBH) and stored in vesicles in the neurons (4). Released NE in synaptic junctions is either inactivated by COMT in postsynaptic cells or transported by a NE transporter (NET) into the nerve terminals (uptake-1). Dopamine is also efficiently transported by NET. At extraneuronal locations, DAT is present in placenta and lung endothelial cells and NET is present in stomach and pancreas. There are also three non-neuronal transporters functioning in peripheral tissues such as the heart, liver, kidney, intestine, blood vessels, retina, and placenta. These uptakes by non-neuronal cells are termed uptake-2.

After transported into sympathetic nerve ending by uptake-1, 6-[^18^F]FDA is rapidly converted to 6-[^18^F]fluoronorepinephrine (6-FNE) by DBH in neuronal vesicles (5). 6-[^18^F]FDA is also metabolized via mitochondrial monoamine oxidase to yield [^18^F]6-fluoro-3,4-dihydroxyphenylacetic acid (FDOPAC). In nonneuronal cells, 6-[^18^F]FDA is converted by COMT sequentially to O-[^18^F]methoxytyramine and [^18^F]6-fluorochomovanillic acid (FHVA). FDOPAC taken up after release from sympathetic neurons by uptake-2 is converted to FHVA by COMT. Uptake of 6-[^18^F]FDA into sympathetic nerve terminals, with conversion to and storage of 6-[^18^F]FNE in vesicles, would lead to more intense positron emission tomography (PET) signals from sympathetically innervated tissues than noninnervated tissues.

### Related Resource Links:

- Chapters in MICAD (Dopamine (http://www.ncbi.nlm.nih.gov/books/?term=Dopamine+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books))
- Gene information in NCBI (Aromatic L-amino acid decarboxylase (http://www.ncbi.nlm.nih.gov/gene/1644), tyrosine hydroxylase (http://www.ncbi.nlm.nih.gov/gene/7054))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Aromatic L-amino acid decarboxylase (http://omim.org/entry/107930), tyrosine hydroxylase (http://omim.org/entry/191290?search=tyrosine%20hydroxylase&highlight=hydroxylase%20tyrosine))
- Clinical trials (6-[^18^F]FDA (http://www.clinicaltrials.gov/ct2/results?term=Fluorodopamine))
- Drug information in FDA (6-[^18^F]FDA (http://google2.fda.gov/search?q=Fluorodopamine&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=15&y=12&sort=date%3AD%3AL%3Ad1&entqr=3&entqrm=0&oe=UTF-8&ie=UTF-8&ud=1&site=FDAgov&btnG=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%226-fluorodopamine%22%5BSubstance%20Name%5D%20AND%20synthesis%5BAll%20Fields%5D)]

6-[^18^F]FDA was synthesized from 6-[^18^F]FDOPA by enzymatic decarboxylation using AAAD prepared from hog kidneys with a radiochemical purity of >98% and a specific activity of 1 mCi/mg (37 MBq/mg) (5). A direct synthesis was also used to produce a higher specific activity. N-(trifluoroacetyl)-3,4-dimethoxy-6-trifluoroacetoxymercuro-β-phenethyamine was fluorodemercurated by [^18^F]F_2_ to form 6-[^18^F]FDA with radiochemical purity of 98% and about 800 mCi/mmol (22 MBq/mmol) at end of synthesis (EOS) (6).

In order to obtain a higher specific activity, a multi-step synthesis of 6-[^18^F]FDA using nucleophilic aromatic substitution by [^18^F]fluoride ion/Kryptofix2.2.2 was achieved in 105 min with a radiochemical yield of 20% and a specific activity of 2-5 Ci/μmol (74-185 GBq/μmol) at end of bombardment (EOB) (7). Chemical and radiochemical purities were >98%.

6-[^18^F]FDA was routinely synthesized by the direct fluorination of dopamine with [^18^F]KF using the standard [^18^F] potassium Kryptofix complex (8). Reverse-phase high-performance liquid chromatography was used to separate 6-[^18^F]FDA from the reaction mixture containing 2- and 5-[^18^F]FDA. The radiochemical yield of 6-[^18^F]FDA was 10 ± 2% at the end of the 120-min synthesis from EOB. The specific activity of 6-[^18^F]FDA was 10 Ci/mmol (370 GBq/mmol) at EOS.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDOPA%5BAll%20Fields%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

The enzyme kinetic parameters using Lineweaver-Burk plots for uptake of [^3^H]DA and 6-[^18^F]FDA were determined in vitro from bovine chromaffin granule membranes (9). The K_m_ and V_max_ values for [^3^H]DA were 14.7 μM and 1.6 nmol/mg protein-min, respectively. The K_m_ and V_max_ values for 6-[^18^F]FDA were 15.3 μM and 2.4 nmol/mg protein-min, respectively. FDA showed an affinity comparable to DA. Both uptakes were inhibited by reserpine, an uptake-1 blocker. Unlabeled FDA inhibited uptake of [^3^H]DA with a K_i_ value of 20.8 μM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%226-fluorodopamine%22%5BSubstance%20Name%5D%20AND%20rodentia)]

High uptake of radioactivity was found in the kidneys, left ventricular myocardium, spleen, salivary gland and liver of rats at 5 min post injection of [^3^H]6-FDA (10). The amount of radioactivity was decreased to less than 3% in plasma in 5 min. Tissue to blood ratios increased progressively from 5 min to 120 min. In the heart, the majority of the tissue radioactivity was [^3^H]6-FDA (17%) and [^3^H]6-FNE (70%). In the kidneys and liver, [^3^H]FDA and [^3^H]FNE contributions were below 30%. No [^3^H]6-FNE was detected in the plasma.

The neuronal uptake and metabolism of 6-[^18^F]FDA and [^3^H]DA were studied in heart, submaxillary gland and spleen. Less 6-[^18^F]FNE accumulation in tissues than [^3^H]NE was observed as a result of inefficient hydroxylation of fluorinated dopamine (11). 6-[^18^F]FDA was rapidly stored in vesicles of sympathetic neurons but was a poorer substrate than [^3^H]DA to form NE. Accumulation of [^3^H]catechols in the heart was decreased by 64-88% when unlabeled 6-FDA (250 μg/kg) was co-injected with trace amount of [^3^H]DA. Desipramine and reserpine (uptake-1 blockers) pretreatment of rats blocked the tissue accumulation of tritiated and fluorinated dopamine and their dihydroxy-metabolites.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FDOPA%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%226-fluorodopamine%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

In dogs, 6-[^18^F]FDA PET images were intense in the renal pelvis, heart, liver, kidneys, spleen and salivary glands, with little signal from the brain, lungs, and skeletal muscle at 1 h post injection (10). Concentrations of radioactivity in blood and plasma fell rapidly with a biologic half-life of 1.5 min. The left ventricular myocardium was strikingly delineated. High radioactivity in the gallbladder and urinary system pointed to the hepatic and renal excretion of the tracer and its metabolites. Treatment with 6-hydroxydopamine (6-OHDA, neurotoxin) or reserpine (uptake-1 blocker) diminished almost completely the signal from the left ventricular myocardium (12). Plasma FDOPAC levels were lowered in 6-OHDA treated dogs and elevated in reserpinized dogs. Decreased PET signal from denervated salivary gland also confirmed that 6-[^18^F]FDA was accumulated normally in sympathetic neurons (5).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-fluorodopamine%20AND%20primate%20NOT%20human)]

Comparative PET studies of (-) and (+)-6-[18F]FNE and of 6-[^18^F]FDA in the heart was performed in the same baboon (13). There was a longer retention of radioactivity after injection of (-)FNE than for the (+)FNE. There was an initially higher and faster uptake in the heart for 6-[^18^F]FDA than for FNE. All three tracers disappeared rapidly in plasma. There was a greater washout also for 6-[^18^F]FDA than for FNE. There was only 1-2% of intact FDA as compared to 28% for (-)FNE and 17% for (+)FNE at 10 min postinjections. Most of the metabolites were methylated non-catechols. Metabolites appeared more rapidly for FDA than (-)FNE and (+)FNE. Desipramine (a specific NET blocker, 0.5 mg/kg) blocked almost completely the uptake of (-)FNE and there was a 60-70% recovery of FNE uptake at 24 hr after desipramine pretreatment. The uptake of 6-[^18^F]FDA was only partially blocked by desipramine at the same dosage suggesting additional reuptake mechanisms for 6-[^18^F]FDA accumulation in the heart.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-fluorodopamine%20AND%20human)]

Human dosimetry was estimated in 10 healthy volunteers (14). The bladder wall receives the highest dose (0.22 mGy/MBq or 0.83 rad/mCi). Other organs receiving high doses are the kidneys (0.19 mGy/MBq or 0.71 rad/mCi) and spleen (0.037 mGy/MBq or 0.14 rad/mCi). The liver and lungs receive <0.016 mGy/MBq (0.06 rad/mCi). Effective dose equivalent of 0.0068 mSv/MBq (25 mrem/mCi) was estimated in the intravenous administration of 6-[^18^F]FDA.

6-[^18^F]FDA PET scans were obtained in healthy volunteers after intravenous injection of 1-4 mCi (37-148 MBq) 6-[^18^F]FDA (15). The left ventricular myocardium was visualized in all subjects. Arterial plasma FDA concentration decreased rapidly with a biologic half-life of 2.4 min. FHVA and FDA-sulfate appeared rapidly in the plasma. No FNE and its metabolites were detected. Greater than 94% of FDA was excreted mostly as metabolites in urine at 24 h after injection. Desipramine (uptake-1 blocker) decreased uptake of myocardial radioactivity and plasma FDOPAC. Trimethaphan (TRI), a postganglion nerve traffic blocker, induced higher levels of 6-[^18^F]FDA PET myocardial signal than untreated subjects. TRI increased FDOPAC plasma levels but decreased FNE levels as compared to untreated subjects. Tyramine (TYR) displaces amines from vesicles and induces release of NE into synaptic cleft. TYR decreased 6-[^18^F]FDA PET myocardial signal more rapidly than untreated subjects. TYR increased plasma levels of FNE and its metabolite by 30% and 78%, respectively. FDA PET scanning is a useful tool to assess sympathetic innervation and function noninvasively in human myocardium.

6-[^18^F]FDA PET permits objective monitoring of cardiac sympathetic innervation and function in various disease conditions, such as PD (16), hypertension and congestive heart failure (17). 6-[^18^F]FDA has also demonstrated its usefulness in the imaging of chromaffin tumors, neuroblastomas, ganglioneuromas and metastatic pheochromocytoma (18, 19).

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Barrio J.R., Huang S.C., Phelps M.E. (1997). Biological imaging and the molecular basis of dopaminergic diseases. Biochem Pharmacol.
4 Eisenhofer G. (2001). The role of neuronal and extraneuronal plasma membrane transporters in the inactivation of peripheral catecholamines. Pharmacol Ther.
5 Goldstein D.S., Chang P.C., Eisenhofer G., Miletich R., Finn R., Bacher J., Kirk K.L., Bacharach S., Kopin I.J. (1990). Positron emission tomographic imaging of cardiac sympathetic innervation and function. Circulation.
6 Goldstein D.S., Eisenhofer G., Dunn B.B., Armando I., Lenders J., Grossman E., Holmes C., Kirk K.L., Bacharach S., Adams R., et al. (1993). Positron emission tomographic imaging of cardiac sympathetic innervation using 6-[18F]fluorodopamine: initial findings in humans. J Am Coll Cardiol.
7 Ding Y.S., Fowler J.S., Gatley S.J., Dewey S.L., Wolf A.P., Schlyer D.J. (1991). Synthesis of high specific activity 6-[18F]fluorodopamine for positron emission tomography studies of sympathetic nervous tissue. J Med Chem.
8 Chirakal R., Coates G., Firnau G., Schrobilgen G.J., Nahmias C. (1996). Direct radiofluorination of dopamine: 18F-labeled 6-fluorodopamine for imaging cardiac sympathetic innervation in humans using positron emission tomography. Nucl Med Biol.
9 Endres C.J., Swaminathan S., DeJesus O.T., Sievert M., Ruoho A.E., Murali D., Rommelfanger S.G., Holden J.E. (1997). Affinities of dopamine analogs for monoamine granular and plasma membrane transporters: implications for PET dopamine studies. Life Sci.
10 Goldstein D.S., Chang P.C., Smith C.B., Herscovitch P., Austin S.M., Eisenhofer G., Kopin I.J. (1991). Dosimetric estimates for clinical positron emission tomographic scanning after injection of [18F]-6-fluorodopamine. J Nucl Med.
11 Eisenhofer G., Hovevey-Sion D., Kopin I.J., Miletich R., Kirk K.L., Finn R., Goldstein D.S. (1989). Neuronal uptake and metabolism of 2- and 6-fluorodopamine: false neurotransmitters for positron emission tomographic imaging of sympathetically innervated tissues. J Pharmacol Exp Ther.
12 Goldstein D.S., Grossman E., Tamrat M., Chang P.C., Eisenhofer G., Bacher J., Kirk K.L., Bacharach S., Kopin I.J. (1991). Positron emission imaging of cardiac sympathetic innervation and function using 18F-6-fluorodopamine: effects of chemical sympathectomy by 6-hydroxydopamine. J Hypertens.
13 Ding Y.S., Fowler J.S., Dewey S.L., Logan J., Schlyer D.J., Gatley S.J., Volkow N.D., King P.T., Wolf A.P. (1993). Comparison of high specific activity (-) and (+)-6-[18F]fluoronorepinephrine and 6-[18F]fluorodopamine in baboons: heart uptake, metabolism and the effect of desipramine. J Nucl Med.
14 Goldstein D.S., Coronado L., Kopin I.J. (1994). 6-[Fluorine-18]fluorodopamine pharmacokinetics and dosimetry in humans. J Nucl Med.
15 Goldstein D.S., Holmes C., Stuhlmuller J.E., Lenders J.W., Kopin I.J. (1997). 6-[18F]fluorodopamine positron emission tomographic scanning in the assessment of cardiac sympathoneural function--studies in normal humans. Clin Auton Res.
16 Li S.T., Dendi R., Holmes C., Goldstein D.S. (2002). Progressive loss of cardiac sympathetic innervation in Parkinson's disease. Ann Neurol.
17 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
18 Ilias I., Shulkin B., Pacak K. (2005). New functional imaging modalities for chromaffin tumors, neuroblastomas and ganglioneuromas. Trends Endocrinol Metab.
19 Goldstein D.S., Eisenhofer G., Flynn J.A., Wand G., Pacak K. (2004). Diagnosis and localization of pheochromocytoma. Hypertension.